# ^124^I-Anti-CD44v6 chimeric monoclonal antibody U36

Chemical name: | ^124^I-Anti-CD44v6 chimeric monoclonal antibody U36
Abbreviated name: | ^124^I-cMAb U36, ^124^I-U36
Synonym:
Agent Category: | Antibody
Target: | CD44v6
Target Category: | Antibody-antigen binding
Method of detection: | PET
Source of signal: | ^124^I
Activation: | No
Studies: | - In Vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=685122), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48255940) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=960) for more information about CD44.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+AND+U36)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

The splice variant v6 of the cell membrane glycoprotein CD44 (CD44v6) is expressed in only a few normal epithelial tissues (e.g., thyroid and prostate gland). CD44 binds to ECM and is associated with cell adhesion, lymphocyte activation, and tumor cell metastasis (4, 5). Elevated levels of CD44v6 have been found in epithelial tumors associated with a poor prognosis for cancer patients (5). U36, an anti-CD44v6 chimeric (mouse/human) monoclonal antibody (cMAb), was found not bind to follicles or C cells from normal human thyroid (6). CD44v6 is generally highly expressed in thyroid carcinoma (7). ^124^I-cMAb U36 was developed for imaging of CD44v6 expression in thyroid carcinomas and other epithelial tumors (8, 9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+AND+U36+synthesis)]

cMAb U36 was labeled with sodium [^124^I]iodide by electrophilic radioiodination via the chloramine-T (8) or Iodogen method (9). ^124^I-cMAb U36 was purified by gel filtration. Both methods provided labeling yields of >70%. The radiochemical purity was >97%. No specific activity values were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+U36+and+in+vitro)]

Fortin et al. (8) reported that high-affinity ^125^I-cMAb U36 binding sites (B_max_ = 570,000 ± 30,000 sites/cell, K_d_ = 11 ± 2 nM) were found on the cell surfaces of KAT-4 human anaplastic thyroid carcinoma cells lacking the sodium iodide symporter. Furthermore, 20% of ^125^I-cMAb U36 accumulated in the cells after 24 h at 37°C. The accumulation was reduced to 1% by excess cMAb U36. The labeled cells retained 29% of radioactivity after incubation in tracer-free medium alone for another 24 h at 37°C. No free ^125^I could be detected in the incubation medium. Verel et al. (9) reported that the immunoreactivity of ^124^I-cMAb U36 was 91.1 ± 3.9%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+U36+and+rodentia)]

Fortin et al. (8) performed biodistribution and scintigraphic studies of ^124^I-cMAb U36 in nude mice bearing KAT-4 tumors in the left flank and the right front leg. The organs with the highest accumulation of ^124^I-cMAb U36 (in percent injected dose per gram (% ID/g)) were the urinary bladder (13.1 ± 4.0), lung (7.0 ± 1.3), heart (5.2 ± 1.3), spleen (4.5 ± 1.4), liver (3.9 ± 0.5), and kidneys (3.8 ± 1.0) at 24 h after injection. ^124^I-cMAb U36 uptake in the flank tumors was 8.2 ± 3.6% ID/g, 13.7 ± 0.7% ID/g, 21.8 ± 2.8% ID/g, and 12.8 ± 5.2% ID/g at 4, 24, 48, and 72 h, respectively. The uptake values in the leg tumors were similar to those of the flank tumors. The radioactivity in the thyroid was <1% ID/g at all time points studied. ^124^I-cMAb U36 exhibited a high blood radioactivity (21.8% ID/g) at 4 h, which gradually decreased to 9.5% ID/g at 72 h. On the other hand, ^124^I-cMAb U36 exhibited a low accumulation in the stomach with 5.1% ID/g at 4 h and 1.0% ID/g at 72 h. Scintigraphic images were obtained in the tumor-bearing mice at 24, 48, and 72 h after ^124^I-cMAb U36 injection. The tumors were clearly visible at all time points with the highest uptakes at 48 h. No blocking experiment was performed.

Verel et al. (9) performed biodistribution and scintigraphic studies in nude mice bearing tumors from the HNX-OE human head and neck tumor cell line. Co-injection of ^124^I-cMAb U36 and ^131^I-cMAb U36 with a similar iodine/MAb molar ratio provided similar tissue uptake values. Selective tumor uptake was confirmed with positron emission tomography imaging at 24, 48, and 72 h, which detected 15 out of 15 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+U36+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+U36+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+U36+and+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Van Hal N.L., Van Dongen G.A., Rood-Knippels E.M., Van Der Valk P., Snow G.B., Brakenhoff R.H. (1996). Monoclonal antibody U36, a suitable candidate for clinical immunotherapy of squamous-cell carcinoma, recognizes a CD44 isoform. Int J Cancer.
5 Heider K.H., Kuthan H., Stehle G., Munzert G. (2004). CD44v6: a target for antibody-based cancer therapy. Cancer Immunol Immunother.
6 Schrijvers A.H., Quak J.J., Uyterlinde A.M., van Walsum M., Meijer C.J., Snow G.B., van Dongen G.A. (1993). MAb U36, a novel monoclonal antibody successful in immunotargeting of squamous cell carcinoma of the head and neck. Cancer Res.
7 Aogi K., Kitahara K., Urquidi V., Tarin D., Goodison S. (1999). Comparison of telomerase and CD44 expression as diagnostic tumor markers in lesions of the thyroid. Clin Cancer Res.
8 Fortin M.A., Salnikov A.V., Nestor M., Heldin N.E., Rubin K., Lundqvist H. (2007). Immuno-PET of undifferentiated thyroid carcinoma with radioiodine-labelled antibody cMAb U36: application to antibody tumour uptake studies. Eur J Nucl Med Mol Imaging.
9 Verel I., Visser G.W., Vosjan M.J., Finn R., Boellaard R., van Dongen G.A. (2004). High-quality 124I-labelled monoclonal antibodies for use as PET scouting agents prior to 131I-radioimmunotherapy. Eur J Nucl Med Mol Imaging.